# [^18^F]SB209670

Chemical name: | [^18^F]SB209670
Abbreviated name:
Synonym:
Agent Category: | Compound
Target: | ET receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20SB209670)]

Endothelin (ET)-1 is a polypeptide of 21 amino acids and contains two disulfide bonds located close to the N-terminus. ET-1 is believed to have an important role in a variety of physiological processes and contributes to the development of diseases such as atherosclerosis, hypertension, chronic heart failure, pulmonary hypertension, acute and chronic renal failure, etc (1-3). All of these effects are mediated through a receptor-ligand interaction. Two ET receptors, ET_A_ and ET_B_, have been identified in mammals (4, 5).Each receptor type is expressed in a variety of tissues and some tissues express both types (6). Various cytokines are known to regulate ET-I expression under physiological conditions (1).

In humans, stimulation of the ET_A_ receptors by ET-I on underlying smooth muscles of the endothelium causes vasoconstriction that leads to an elevation of blood pressure and the development of hypertension (7, 8). Stimulation of the ET_B_ receptors on the endothelium itself results in the release of nitric oxide and prostacyclins, which culminates in vasodilation (9). Because of the involvement of ET-I in a variety of physiological processes in both normal and diseased states, it is necessary to elucidate the exact in vivo role of the ET receptor system.

Positron emission tomography (PET) is a very sensitive technique, and recent improvements in equipment design have enabled researchers to use it for investigation of the ET receptor system in a small animal model (9-12). The ^18^F-labeled SB209670 ([^18^F]SB209670) ligand was developed to investigate tissue distribution of ET receptors using PET (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20SB209670%20synthesis)]

The ^18^F analog of SB209670 was produced by alkylation of its precursor SB421672 with 3-[^18^F]fluoropropyl bromide that was prepared with ^18^F-labeled fluoride and 1,3-dibromopropane as described by Johnstrom et al. (9). The final product was purified by reverse-phase high-performance liquid chromatography and the solvent was evaporated for formulation in phosphate-buffered saline.

Labeled SB209670 was synthesized in 162 ± 7 min (n = 6) with a radiochemical yield of 14.9 ± 3.8% and a specific activity of 100–150 GBq/µmol (2.7–4.05 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20SB209670%20in%20vitro)]

The in vitro characterization of [^18^F]SB209670 was performed with human heart left ventricle and kidney tissues (9). For the association experiment, left ventricle sections were incubated with [^18^F]SB209670 for increasing time( 0–120 min) and the saturation assays were performed with increasing concentrations of [^18^F]SB209670 (3 pM to 10 nM) for 60 min. For the competition study, heart and kidney sections were co-incubated with a fixed concentration of [^18^F]SB209670 and either 1 µM FR139317, an ET_A_-selective antagonist, or BQ3020, (an ET_B_-selective antagonist.

Binding of [^18^F]SB209670 to the heart was concentration-dependent and saturable with a dissociation constant (K_D_) of 0.67 ± 0.14 nM, a B_max_ of 168 ± 29.3 fmol/mg protein, and a Hill slope (nH) of 1.07 ± 0.17. The binding was time-dependent with a half-life for association (t_1/2_) of 3.8 min and an association rate constant (k_obs_) of 0.182 ± 0.032/min. This showed that the radioligand retained subnanomolar affinity for the ET receptor in the heart.

Binding of [^18^F]SB209670 could be inhibited partially in the kidney and almost completely in the heart by FR139317, an ET_A_-selective anatagonist, but not by BQ3020, an ET_B_-selective antagonist. Data from this experiment suggests that [^18^F]SB209670 binds primarily to the ET_A_ receptor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20SB209670%20rodentia)]

Rats

In vivo imaging was performed in two Sprague-Dawley rats weighing 260 and 320 g, respectively (9). The animals were administered a bolus injection of 17.1 and 50.8 MBq [^18^F]SB209670, respectively. Specific activity of the radiotracer was ~100 GBq/µmol (2.7 Ci/ µmol) at the time of injection. PET scans were obtained for up to 120 min after injection. At the end of scanning, the animals were euthanized for ex vivo analysis of organs to determine weight and total incorporated radioactivity.

Imaging data revealed that the liver rapidly removed [^18^F]SB209670 from circulation with a peak at 2.5 min, then showed a fast washout that leveled to a steady state after ~50 min with no further decrease for up to 120 min. Subsequently, an increase in uptake was observed in the duodenum and jejunum of the small intestine. Uptake was also observed in the heart (data was obtained between 31 and 120 min). There was an initial increase followed by a decrease for up to 20 min, after which the label reached a steady state. Ex vivo analysis of the liver and intestine confirmed uptake by the liver and excretion primarily through the small and large intestine route. Tissue sections showed localized distribution of radioactivity in the lung, and no uptake was evident in the brain.

Observations made during in vivo scanning suggested a rapid metabolism of [^18^F]SB209670 by the liver, concentration of metabolites in the bile, and excretion into the small intestine. Uptake by the heart suggests binding of SB209670 to the ET_A_ receptors. An ex vivo analysis of the lung sections revealed the binding of labeled SB209670 mainly to the vasculature that is known to contain predominantly ET_A_ receptors. This observation was similar to an observation made earlier with ^18^F-labeled ET-I (10) after the ET_B_ receptors were blocked with BQ788, an antagonist that is selective for these receptors.

### Other Non-Primate Mammals

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20SB209670%20non-primate%20mammals)

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20SB209670%20non-human%20primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20SB209670%20human%20studies)]

No publications are currently available.

## References

1 Kedzierski RM, Yanagisawa M. (2001). Endothelin system: the double-edged sword in health and disease. Annu Rev Pharmacol Toxicol.
2 Miyauchi T, Masaki T. (1999). Pathophysiology of endothelin in the cardiovascular system. Annu. Rev. Physiol.
3 Schiffrin EL, Intengan HD, Thibault G, Touyz RM. (1997). Clinical significance of endothelin in cardiovascular disease. Curr Opin Cardiol.
4 Arai H, Hori S, Aramori I, Ohkubo H, Nakanishi S. (1990). Cloning and expression of a cDNA encoding an endothelin receptor. Nature.
5 Sakurai T, Yanagisawa M, Takuwa Y, Miyazaki H, Kimura S, Goto K, Masaki T. (1990). Cloning of a cDNA encoding a non-isopeptide-selective subtype of the endothelin receptor. Nature.
6. Davenport, AP, Distribution of endothelin receptors. Endothelins in biology and medicine., ed. JP Huggins and JT Pelton. 1997, Boca Raton: CRC Press, Inc. 45-68.
7 de Nucci G, Thomas GR, D'Orleans-Juste P, Antunes E, Walder C, Warner TD, Vane JR. (1988). Pressor effects of circulating endothelin are limited by its removal in primary circulation and by the release of prostacyclin and endothelium-derived relaxing factor. Proc. Natl. Acad. Sci. USA.
8 Yokokawa K, Tahara H, Kohno M, Murakawa K, Yasunari K, Nakagawa K, Hamada T, Otani S, Yanagisawa M, Takeda T. (1991). Hyperstension associated with endothelin secreting malignant hemangioendothelioma. Ann Intern Med.
9 Johnstrom P, Fryer TD, Richards HK, Barret O, Clark JC, Ohlstein EH, Pickard JD, Davenport AP. (2004). In Vivo Imaging of Cardiovascular Endothelin Receptors Using the Novel Radiolabelled Antagonist [18F]-SB209670 and Positron Emission Tomography (microPET). J Cardiovasc Pharmacol.
10 Johnstrom P, Fryer TD, Richards HK, Harris NG, Barret O, Clark JC, Pickard JD, Davenport AP. (2005). Positron emission tomography using 18F-labelled endothelin-1 reveals prevention of binding to cardiac receptors owing to tissue-specific clearance by ET B receptors in vivo. Br J Pharmacol.
11 Johnstrom P, Harris NG, Fryer TD, Barret O, Clark JC, Pickard JD, Davenport AP. (2002). (18)F-Endothelin-1, a positron emission tomography (PET) radioligand for the endothelin receptor system: radiosynthesis and in vivo imaging using microPET. Clin Sci (Lond).
12 Johnstrom P, Rudd JH, Richards HK, Fryer TD, Clark JC, Weissberg PL, Pickard JD, Davenport AP. (2006). Imaging endothelin ET(B) receptors using [18F]-BQ3020: in vitro characterization and positron emission tomography (microPET). Exp Biol Med (Maywood).